# Cyclo(Arg-Gly-Asp-D-Tyr-Lys)-Cy5.5

Chemical name: | Cyclo(Arg-Gly-Asp-D-Tyr-Lys)-Cy5.5
Abbreviated name: | RGD-Cy5.5
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor
Method of detection: | Optical, Near-Infrared (NIR) fluorescence imaging
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D)]

Integrins are a family of cell surface heterodimeric glycoproteins that mediate diverse biological events involving cell-cell and cell-matrix interactions (1). They consist of an α and a β subunit. They are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (2-7). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as anti-tumor and anti-angiogenic agents (4, 8, 9) and the agonists as angiogenic agents for coronary angiogenesis (10, 11). A tripeptide sequence consisting of Arg-Gly-Asp (RGD) is identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins including α_v_β_3_. Various radiolabeled antagonists were introduced for imaging of tumors and tumor angiogenesis (12).

Optical fluorescence imaging is increasingly used to obtain biological functions of specific targets (13, 14). However, the intrinsic fluorescence of biomolecules poses a problem when visible light (350-700 nm) absorbing fluorophores are used. Near-infrared (NIR) fluorescence (700-1000 nm) detection avoids the background fluorescence interference of natural biomolecules, providing a high contrast between target and background tissues. NIR fluorophores have wider dynamic range and minimal background as a result of reduced scattering compared with visible fluorescence detection. They also have high sensitivity, resulting from low infrared background, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is becoming a non-invasive alternative to radionuclide imaging.

Cyclo(RGDyK) was conjugated with Cy5.5 to study in vivo biodistribution of the tracer in tumor-bearing mice. Cy5.5 is a NIR fluorescent dye with absorbance maximum at 675 nm and emission maximum at 694 nm with a high extinction coefficient of 250,000 (mol/L)^-1^cm^-1^. RGD-Cy5.5 or c(RGDyK)-Cy5.5 was found to have a high and long-lasting accumulation in α_v_β_3_-positve U87MG human glioblastoma tumor cells in nude mice (15). The binding of RGD-Cy5.5 to the integrin receptor was found to be specific both in vitro and in vivo.

### Related Resource Links:

- Chapters in MICAD (RGD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=RGD+AND+micad%5Bbook%5D))
- Gene information in NCBI (α_v_ integrin (http://www.ncbi.nlm.nih.gov/gene/3685), β_3_ integrin (http://www.ncbi.nlm.nih.gov/gene/3690))
- Articles in Online Mendelian Inheritance in Man (OMIM) (α_v_ integrin (http://www.ncbi.nlm.nih.gov/omim/193210), β_3_ integrin (http://www.ncbi.nlm.nih.gov/omim/173470))
- Clinical trials (RGD (http://www.clinicaltrials.gov/ct2/results?term=RGD))
- Drug information in FDA (RGD (http://google2.fda.gov/search?q=RGD&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=12&y=8))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5Dand%20synthesis)]

Cy5.5 monofunctional N-hydroxysuccinimide (NHS) ester was used to conjugate c(RGDyK) to form c(RGDyK)-Cy5.5, which was purified by high-performance liquid chromatography (15). A chemical yield of 70-75% was obtained. The NHS ester of Cy5.5 is reacted with the ε-amino group of the lysine in c(RGDyK). The peak containing the RGD-Cy5.5 conjugate was analyzed by matrix-assisted laser desorption/ionization-time-of-flight mass spectrometry (MALDI-TOF MS). The measured mass (m/z, 1518.4) was the same as the expected mass (m/z, 1518.7).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20%28%22in%20vitro%22%5BMeSH%20Terms%5D%20OR%20in%20vitro%5BText%20Word%5D%29)]

A receptor-binding assay with ^125^I-labeled c(RGDyK) (0.06 nM) was established using immobilized α_v_β_3_ receptors on plastic microtiter plate wells. RGD-Cy5.5 and c(RGDyK) had an IC_50_ of 58.1 and 37.5 nM, respectively (15). Receptor-mediated endocytosis of RGD-Cy5.5 in U87MG tumor cells and HBCEC human brain endothelial cells was observed by confocal laser-scanning microscopy. Binding of 100 nM RGD-Cy5.5 to both cell types was completely blocked by 10 μM c(RGDyK).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Biodistribution studies of RGD-Cy5.5 were evaluated in nude mice using a U87MG glioblastoma subcutaneous xenograft model (15). U87MG tumor cells were injected subcutaneously into the right foreleg. Images were obtained at 10 min, 30 min, 1 h, 2 h, 4 h and 24 h postinjection of 0.5 nmol RGD-Cy5.5. The tumor uptake of RGD-Cy5.5 could be clearly seen from 30 min to 24 h. A maximal uptake in the tumor was reached at 2 h and slowly washed out over time. The tracer uptake could be blocked by co-injection of 100 nmol c(RGDyK). This proves to be a noninvasive imaging of tumor cells in mice by using optical technique.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%5D%20AND%20%28dog%20or%20pig%20or%20rabbit%20or%20sheep%29)]

No publication is currently available

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20primates%20NOT%20humans)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=RGD%5BAll%20Fields%5D%20AND%20%22CY5.5%20cyanine%20dye%22%5BSubstance%20Name%5D%20AND%20humans%20not%20cell%20line)]

No publication is currently available.

## Reference

1 Hynes R.O., Lively J.C., McCarty J.H., Taverna D., Francis S.E., Hodivala-Dilke K., Xiao Q. (2002). The diverse roles of integrins and their ligands in angiogenesis. Cold Spring Harb Symp Quant Biol.
2 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
3 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
4 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
5 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
6 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
7 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
8 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
9 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
10 Sadeghi M.M., Krassilnikova S., Zhang J., Gharaei A.A., Fassaei H.R., Esmailzadeh L., Kooshkabadi A., Edwards S., Yalamanchili P., Harris T.D., Sinusas A.J., Zaret B.L., Bender J.R. (2004). Detection of injury-induced vascular remodeling by targeting activated alphavbeta3 integrin in vivo. Circulation.
11 Sinusas A.J. (2004). Imaging of angiogenesis. J Nucl Cardiol.
12 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
13 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
14 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
15 Chen X., Conti P.S., Moats R.A. (2004). In vivo near-infrared fluorescence imaging of integrin alphavbeta3 in brain tumor xenografts. Cancer Res.